# ^111^Indium-diethylenetriaminepentaacetic acid-folate

Chemical name: | ^111^Indium-diethylenetriaminepentaacetic acid-folate
Abbreviated name: | ^111^In-DTPA-folate
Synonym: | ^111^In-P3139
Agent category: | Compound
Target: | Folic acid receptor
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22DTPA%20folate%22%5BSubstance%20Name%5D)]

Folic acid is a water-soluble B vitamin (1). It is essential for methylation and DNA synthesis. The primary pathway for entry of folate into cells is through facilitated transporter, which has a low affinity for folate with K_m_ of 1-5 μM. Some cells in choroid plexus, kidney, lung, thyroid, spleen, placenta, and thymus also possess a high affinity (K_d_, 0.5 nM) receptor that allows folate retention via receptor-mediated endocytosis. Some human epithelial tumor cells were found to overexpress folate-binding protein (2). More than 90% of human ovarian and endometrial cancers express the high-affinity receptor, which is absent in the normal tissues. Breast, colorectal, renal, and lung carcinomas also over-expressed the folate receptor but to a lesser frequency (20-50%). Several folate-based conjugates have been studied in tumor imaging. ^111^In-DTPA-folate was synthesized and developed as a folate receptor imaging agent (3). It was recently shown to be a useful imaging agent in diagnosis of human benign ovarian cancer (4).

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=folate+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (folate receptor (http://www.ncbi.nlm.nih.gov/gene/2348))
- Articles in OMIM (folate receptor (http://www.ncbi.nlm.nih.gov/omim/136430))
- Clinical trials (folate receptors (http://www.clinicaltrials.gov/ct2/results?term=folate+receptor))
- Drug information in FDA (http://google2.fda.gov/search?q=folate+receptor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=14&y=15)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22DTPA%20folate%22%5BSubstance%20Name%5D%20AND%20synthesis%5BAll%20Fields%5D)]

^111^In-DTPA-folate was obtained in high radiochemical yield by ligand exchange from ^111^In-citrate with DTPA-folate providing a chemical purity of >92% (3). The specific activity was about 16 μCi/μg (0.6 MBq/μg). DTPA-folate was characterized by analytical HPLC, mass spectroscopy, and NMR. A molar ratio of DTPA to folate of 1:1 was identified.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22DTPA%20folate%22%5BSubstance%20Name%5D%20AND%20cell%20line)]

Human nasopharyngeal carcinoma KB cells have a K_d_ of 1.6 nM for FITC-folate (3). Cellular uptake of 100 nM ^111^In-DTPA-folate was saturable within 10 min of incubation at room temperature and was completely blocked by 1 mM folate. A549 cells (folate-receptor negative) did not show any specific uptake of ^111^In-DTPA-folate.

Kinetics of receptor-mediated endocytosis of [^3^H]folate, FITC-folate and ^111^In-DTPA-folate was studied in a panel of six folate receptor-positive (3-18 X10^6^ folate per cell) cancer cells (5). All three folate conjugates (50 nM) associated with the cells and approached saturation within 30 min. The rate of internalization (1-3 X 10^5^ molecules/h) for all three folate conjugates was the same for all cells indicating that the rate of internalization is not dependent on folate binding capacity. ^111^In-DTPA-folate was internalized as efficiently as [^3^H]folate. Only 10 to 25% of the total cell-bound radioactivity was internalized at 6 h of incubation. The data suggest that most of the folate conjugates either remain on the cell surface or recycle without unloading inside the cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22DTPA%20folate%22%5BSubstance%20Name%5D%20AND%20rodentia)]

Following intravenous administration to normal rats, the ^111^In-DTPA-folate radiotracer was found to be efficiently cleared from the blood and primarily excreted into the urine at 4 h postinjection (3). The organ with the highest uptake was the kidneys, followed by the intestines, liver, and urinary bladder. A folate receptor-positive KB cell tumor transplanted in a nude mouse was readily visualized by scintigraphy 1 h following intravenous administration of ^111^In-DTPA-folate.

Nude mice were inoculated with KB tumor cells, followed by intravenous injection of (200 μCi/mouse, 7.4 MBq/mouse, 17 μg/mouse) ^111^In-DTPA-folate 15 days after tumor transplantation (6). The tumor uptake of ^111^In-DTPA-folate was 3.1%ID/g at 4 h postinjection. The tumor-to-blood, tumor-to-liver, tumor-to-kidney and tumor-to-muscle ratios were 346, 31, 1, and 33.3, respectively. Co-injection with 205 μmol/kg unlabeled folate blocked the tumor uptake by 90%. Delaying the injection of unlabeled folate by 3 h after the tracer injection the tumor uptake was only reduced by 22%, suggesting the tracer had mostly been internalized by the tumor cells. The tumor uptake was found to increase from 1 to 30 min and then stabilized from 30 min to 24h postinjection. Tumor uptakes of ^111^In-DTPA and ^111^In-citrate were negligible.

Mice were subcutaneously implanted with L1210A, M109, and Line 01 tumors, followed by injections of 50 to 4000 nmol/kg of ^111^In-DTPA-folate. The three tumors and kidneys all saturated at concentrations of about 2000 nmol/kg. L1210A had the highest uptake, followed by the kidneys, M109 and Line 01. The rate of folate receptor recycling was estimated to be <5.7 h for L1210A, but 13.3 to 20 h for Line 01 and M109 cells. Recycling in the kidney was about 5.7 h. The other normal tissues such as the heart, lung, liver, spleen, intestine, and muscle express fewer folate receptors than the tumor cells; they still recycled their receptors near 8 h. The retention time of a saturable dose of ^111^In-DTPA-folate in tumor-bearing mice was studied. The unloading rates of ^111^In-DTPA-folate (about 5.2-6.2 X10^-3^ nmol/kg/h) were similar for all tumors and the kidney. Although other normal tissues have much lower uptake of ^111^In-DTPA-folate, their unloading rates are similar to the tumors and kidney.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22DTPA%20folate%22%5BSubstance%20Name%5D%20and%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DTPA-folate%20AND%20primate%20NOT%20human)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DTPA-folate%20AND%20human)]

^111^In-DTPA-folate was evaluated for diagnosis of ovarian cancer in women (4). Imaging was performed 4 h post injection of 185 MBq (5 mCi). Among 33 patients who had surgical intervention, 14 had new or recurrent malignant tumors. All of 7 newly diagnosed ovarian carcinomas were identified by both masked and unmasked readers (sensitivity, 100%). The sensitivity for detection of 7 recurrent tumors was 38% for masked readings and 85% for unmasked readings, indicating that correlation with anatomic imaging studies by computer tomography was highly important in diagnosis of these lesions. Eighteen of the studied patients were found to have benign lesions; the specificity of ^111^In-DTPA-folate scintigraphy was 76% and 82% for the masked and unmasked analyses, respectively. Therefore, ^111^In-DTPA-folate is safe and effective for scintigraphy differentiating between malignant and benign ovarian lesions.

## NIH Support

P30-CA23168, R01-CA70845, R43 CA73260

## References

1 Stanger O. (2002). Physiology of folic acid in health and disease. Curr Drug Metab.
2 Ke C.Y., Mathias C.J., Green M.A. (2003). The folate receptor as a molecular target for tumor-selective radionuclide delivery. Nucl Med Biol.
3 Wang S., Luo J., Lantrip D.A., Waters D.J., Mathias C.J., Green M.A., Fuchs P.L., Low P.S. (1997). Design and synthesis of [111In]DTPA-folate for use as a tumor-targeted radiopharmaceutical. Bioconjug Chem.
4 Siegel B.A., Dehdashti F., Mutch D.G., Podoloff D.A., Wendt R., Sutton G.P., Burt R.W., Ellis P.R., Mathias C.J., Green M.A., Gershenson D.M. (2003). Evaluation of 111In-DTPA-folate as a receptor-targeted diagnostic agent for ovarian cancer: initial clinical results. J Nucl Med.
5 Paulos C.M., Reddy J.A., Leamon C.P., Turk M.J., Low P.S. (2004). Ligand binding and kinetics of folate receptor recycling in vivo: impact on receptor-mediated drug delivery. Mol Pharmacol.
6 Mathias C.J., Wang S., Waters D.J., Turek J.J., Low P.S., Green M.A. (1998). Indium-111-DTPA-folate as a potential folate-receptor-targeted radiopharmaceutical. J Nucl Med.